# ^124^I-Serum albumin-manganese-magnetism-engineered iron oxide nanoparticles

Chemical name: | ^124^I-Serum albumin-manganese-magnetism-engineered iron oxide nanoparticles
Abbreviated name: | ^124^I-SA-MnMEIO
Synonym:
Agent category: | Nanoparticle
Target: | Unknown
Target category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI), positron emission tomography (PET)
Source of signal\contrast: | Iron oxide, ^124^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20MRI)]

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or other polysaccharide. These particles have large combined magnetic moments or spins that are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in magnetic resonance imaging (MRI), though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system is by endocytosis or phagocytosis. SPIO particles are taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. (1). SPIO agents are classified by their sizes with coating material (~20 nm to 3,500 nm in diameter) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultra small SPIO (USPIO) nanoparticles, and cross-linked iron oxide (CLIO) nanoparticles. A new class of iron oxide nanoparticles has been created with high and tunable nanomagnetism: magnetism-engineered iron oxide (MEIO) nanoparticles (2). These MEIO nanoparticles were doped with manganese (MnMEIO) to provide further MRI signal enhancement.

The sentinel lymph node (SLN) is considered to be the first lymph node to receive lymphatic flow from tumor sites and thus will contain metastatic tumor cells (3). SLN mapping has been used in the diagnosis of metastasis of solid tumors (4). Radical lymph node dissection is performed in patients with malignant cells in the SLNs. SLN mapping is currently performed with a combination of radioactive tracer and blue dye. The current procedure is also time-consuming and requires a steep learning curve. Near-infrared quantum dots have been studied in SLN mapping in small animals (5, 6); however, there are only limited studies of long-term quantum dot toxicity in animals (7). Choi et al. (8) have designed a multimodal magnetic nanoparticle-based positron emission tomography (PET)/MRI probe for non-invasive mapping of SLNs in small animals. MnMEIO was coated with serum albumin (SA) and radiolabeled with ^124^I to form ^124^I-SA-MnMEIO nanoparticles.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20MRI%20and%20synthesis)]

SA-MnMEIO nanoparticles were cross-linked in the presence of N-(3-dimethylaminopropyl)-N-ethylcarbodiimide hydrochloride and N-hydroxysulfosuccinimide for 2 h at room temperature (8). The cross-linked SA-MnMEIO nanoparticles were purified with gel filtration chromatography and labeled with 37 MBq (1 mCi) ^124^I in the presence of Iodobeads for 15 min. ^124^I-SA-MnMEIO nanoparticles were purified with centrifugation, and the radiochemical purity was >92% with a specific activity of 51.8 MBq/mg (1.4 mCi/mg) at the time of injection. ^124^I-SA-MnMEIO nanoparticles exhibited a hydrodynamic diameter of ~32 nm (core diameter, ~15 nm) and a T2 relaxivity coefficient r_2_ of 321.6 mM^-1^s^-1^ measured at 1.5 T.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20MRI%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20MRI%20and%20rodentia)]

Choi et al. (8) used PET and MRI imaging to measure ^124^I-SA-MnMEIO nanoparticle (80 μg) accumulation in the lymph nodes of rats after subcutaneous injection into the right front paw. The brachial lymph node (the first lymph node encountered) was visible in both the PET and the MRI images 1 h after injection. However, the precise positioning of the brachial lymph node and an additional deeper axillary lymph node were obtained only by overlaying the PET and MRI images. The accumulation of ^124^I-SA-MnMEIO nanoparticles reached a peak by 24 h with long-term MRI studies and declined thereafter. ^124^I-SA-MnMEIO accumulation in the brachial lymph nodes was confirmed with ex vivo PET and MRI imaging of the dissected lymph nodes.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20MRI%20and%20(Rabbit+dog+sheep+pig))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20MRI%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MEIO%20MRI%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Lee J.H., Huh Y.M., Jun Y.W., Seo J.W., Jang J.T., Song H.T., Kim S., Cho E.J., Yoon H.G., Suh J.S., Cheon J. (2007). Artificially engineered magnetic nanoparticles for ultra-sensitive molecular imaging. Nat Med.
3 Morton D.L., Wen D.R., Wong J.H., Economou J.S., Cagle L.A., Storm F.K., Foshag L.J., Cochran A.J. (1992). Technical details of intraoperative lymphatic mapping for early stage melanoma. Arch Surg.
4 Schulze T., Bembenek A., Schlag P.M. (2004). Sentinel lymph node biopsy progress in surgical treatment of cancer. Langenbecks Arch Surg.
5 Frangioni J.V., Kim S.W., Ohnishi S., Kim S., Bawendi M.G. (2007). Sentinel Lymph Node Mapping With Type-II Quantum Dots. Methods Mol Biol.
6 Zimmer J.P., Kim S.W., Ohnishi S., Tanaka E., Frangioni J.V., Bawendi M.G. (2006). Size series of small indium arsenide-zinc selenide core-shell nanocrystals and their application to in vivo imaging. J Am Chem Soc.
7 Pinaud F., Michalet X., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Iyer G., Weiss S. (2006). Advances in fluorescence imaging with quantum dot bio-probes. Biomaterials.
8 Choi J.S., Park J.C., Nah H., Woo S., Oh J., Kim K.M., Cheon G.J., Chang Y., Yoo J., Cheon J. (2008). A hybrid nanoparticle probe for dual-modality positron emission tomography and magnetic resonance imaging. Angew Chem Int Ed Engl.